# ^99m^Tc-Labeled mapatumumab

Chemical name: | ^99m^Tc-Labeled mapatumumab
Abbreviated name: | ^99m^Tc-EC-HGS-ETR1
Synonym:
Agent Category: | Antibody
Target: | Tumor necrosis factor–related apoptosis-inducing ligand receptor 1 (TRAIL-R1)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the nucleotice, protein and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=8743&log$=databasead&logdbfrom=protein#refseq) information regarding TRAIL receptors.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1)]

Although anti-growth factor antibodies (Abs) are available for the treatment of cancers (1-3), another technique under investigation to treat this disease is the use of tumor necrosis factor–related apoptosis-inducing ligand (TRAIL) receptor (TRAIL-R) agonist Abs such as mapatumumab and lexatumumab (4, 5). These antibodies (Abs) activate a complex apoptotic pathway in the tumor cell, thereby inducing cell death.The apoptotic pathway and the four TRAIL-R types in humans (designated 1 through 4) have been described in detail by Johnstone et al. (4) and Ashkenazi (5). Mapatumumab (TRM-1 or HGS-ETR1) is a TRAIL-R1 monoclonal antibody (mAb) that targets TRAIL-R1; it is under commercial development and has been approved for clinical trials (http://clinicaltrials.gov/ct2/results?term=Mapatumumab) by the United States Food and Drug Administration (USFDA) to treat various cancers. A similar mAb, lexatumumab (TRM-2 or HGS-ETR2), is a TRAIL-R2 mAb that acts as an agonist specifically for the TRAIL-R2 and has been approved by the USFDA for clinical trials (http://clinicaltrials.gov/ct2/results?term=lexatumumab).

Paclitaxel and docetaxel are anti-cancer drugs that inhibit the mitosis and proliferation of cells by interfering with the depolymerization of microtubules. The mechanism of action of these drugs was discussed in detail by Saloustros et al. (6). Gong et al. observed that the anti-tumor activity of HGS-ETR1 could be enhanced in mice bearing colorectal cancer cell xenograft tumors with pretreatment with paclitaxel (7). Using HGS-ETR1 labeled with radioactive technetium (^99m^Tc) (^99m^Tc-EC-HGS-ETR1), the investigators determined that the activity of HGS-ETR1 was increased because the pretreatment with paclitaxel upregulated the expression of TRAIL-R1 in Colo205 cell xenograft tumors in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of ^99m^Tc-EC-HGS-ETR1 was described by Gong et. al. (7). Briefly, ethylenedicysteine (EC) was coupled to HGS-ETR1 for the chelation of ^99m^Tc using sulfo-N-hydroxysuccinimide (NHS) and 1-ethyl-3-(3-dimethylaminopropyl)carbodiimide hydrochloride (EDC) as the coupling agents. To do this, EC, NHS, and EDC were mixed with HGS-ETR1 and incubated for 17 h at room temperature. The product, EC-HGS-ETR1, was dialyzed (buffer not described) to remove any unbound reagents. The purification, the number of EC per HGS-ETR1, and the yield of EC-HGS-ETR1 were not described by the investigators. Labeling of EC-HGS-ETR1, to obtain ^99m^Tc-EC-HGS-ETR1, was performed by adding sodium pertechnetate (^99m^TcO_4_^-^) to a solution of EC mAb in the presence of tin chloride. The purification and yield of the radiolabeled product were not reported. Although the radiochemical purity of ^99m^Tc-EC-HGS-ETR1 was reported to be >95% (determined with radio thin-layer chromatography), the specific activity of the labeled mAb was not reported.

For use as controls during scintigraphic imaging, ^99m^Tc-EC-bovine serum albumin (BSA) and ^99m^Tc-EC-isotype control mAb were also generated as described above (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+in+vitro)]

The steady state levels of TRAIL-R1 and TRAIL-R2 were determined in Colo205 (a human colorectal cancer tumor cell line) and PA-1 (a human ovarian cancer cell line) cells using immunoblots and fluorescence-activated cell sorting (FACS) (7). Both receptor types were expressed in the two cell lines as determined with the immunoblots, but the levels were reported to be higher in the Colo205 cells than in the PA-1 cells. Similar results were obtained with FACS analysis of the two cell lines.

The concentration for 50% inhibition of cell proliferation (IC_50_) for Colo205 cells was determined to be 800 ng/mL and 150 ng/mL for HGS-ETR1 and HGS-ETR2, respectively (7). The PA-1 cells were reported to be resistant to inhibition by both the Abs even at a concentration of 800 ng/mL. This indicated that the number of TRAIL-R1 and -R2 on the cell surface was too low to initiate apoptosis on binding of the two respective agonist TRAIL-R mAbs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+rodentia)]

Gong et al. studied the tumor uptake of ^99m^Tc-EC-HGS-ETR1 in nude mice bearing Colo205 xenograft tumors (7). Imaging studies were performed 12 days after inoculation with the cells when the tumor diameter was ~1 cm. The animals (4 or 5 mice/group) were intravenously (IV) injected with either ^99m^Tc-EC-HGS-ETR1, ^99m^Tc-EC-BSA, or the ^99m^Tc-EC-isotype control mAb, and scintigraphic images were obtained 2, 24, and 48 h later. Using computer-outlined regions of interest, the counts per pixel of the tumor site and the normal muscle were used to obtain the tumor/muscle count density ratios (TM ratio). At 2 h after administration of the radiochemicals, little difference in the TM ratios was noted between the controls and the ^99m^Tc-EC-HGS-ETR1–treated animals. However, at 24 and 48 h after the injection of radioactivity, the TM ratios for the ^99m^Tc-EC-HGS-ETR1 and the labeled control-injected animals was reported to be ~3 and ~2, respectively. No blocking studies were reported.

In another study, the Colo205 cell xenograft tumor–bearing animals (n = 3 mice) were imaged before and after (at 2 and 24 h after an IV injection of ^99m^Tc-EC-HGS-ETR1) treatment with paclitaxel (7). Animals treated with paclitaxel were imaged 24 h after administration of the drug. When imaging was performed at 2 h after treatment with the labeled mAb, little difference in the TM ratio (~2) was noted in the tumors with or without the paclitaxel treatment. By 24 h the TM ratio was reported to have increased to ~4.2 in tumors of mice treated with paclitaxel compared with a TM ratio of ~2 in the untreated mice. In the same study, PA-1 cell xenograft tumors in animals (n = 3 mice) showed little change in the TM ratio (~1.5) both at 2 and 24 h after the ^99m^Tc-EC-HGS-ETR1 injection. This indicated that very little of the labeled mAb bound to the tumors derived from the PA-1 cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+EC+HGS+ETR1+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Chase J.L. (2008). Clinical use of anti-vascular endothelial growth factor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
2 Patel D.K. (2008). Clinical use of anti-epidermal growth factor receptor monoclonal antibodies in metastatic colorectal cancer. Pharmacotherapy.
3 Sachdev D., Singh R., Fujita-Yamaguchi Y., Yee D. (2006). Down-regulation of insulin receptor by antibodies against the type I insulin-like growth factor receptor: implications for anti-insulin-like growth factor therapy in breast cancer. Cancer Res.
4 Johnstone R.W., Frew A.J., Smyth M.J. (2008). The TRAIL apoptotic pathway in cancer onset, progression and therapy. Nat Rev Cancer.
5 Ashkenazi A. (2008). Directing cancer cells to self-destruct with pro-apoptotic receptor agonists. Nat Rev Drug Discov.
6 Saloustros E., Mavroudis D., Georgoulias V. (2008). Paclitaxel and docetaxel in the treatment of breast cancer. Expert Opin Pharmacother.
7 Gong J., Yang D., Kohanim S., Humphreys R., Broemeling L., Kurzrock R. (2006). Novel in vivo imaging shows up-regulation of death receptors by paclitaxel and correlates with enhanced antitumor effects of receptor agonist antibodies. Mol Cancer Ther.